# ^99m^Tc-Hydrazinonicotinic acid-Glu-{Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_}_2_

Chemical name: | ^99m^Tc-Hydrazinonicotinic acid-Glu-{Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_}_2_
Abbreviated name: | ^99m^Tc-HYNIC-E{E[c(RGDfK)]_2_}_2_
Synonym:
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | SPECT, gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell-cell and cell-matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents and the agonists as angiogenic agents for coronary angiogenesis (6, 8, 9). Extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) contain a tripeptide sequence consisting of Arg-Gly-Asp (RGD), which binds to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most of the cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (IC_50_, 7-40 nM) but not to α_v_β_5_ (IC_50_, 600-4,000 nM) or α_IIb_β_3_ (IC_50_, 700-5,000 nM) integrins. Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). Hydrazinonicotinic acid (HYNIC) is a coupling agent for ^99m^Tc labeling of peptides that can achieve high specific activities without affecting receptor-binding ability of the amino acid sequence. Liu et al. (13) reported the success of radiolabeling cylco(Arg-Gly-Asp-D-Phe-Lys) (c(RGDfK)) tetramer linked by glutamic acid that was conjugated with HYNIC. Trisodium triphenylphosphine-3,3’,3’’-trisulfonate (TPPTS) and tris(hydroxymethyl)-methylglycine (tricine) were used as coligands. ^99m^Tc-HYNIC-E{E[c(RGDfK)]_2_}_2_(tricine)(TPPTS) showed high tumor accumulation in nude mice bearing human tumor xenografts.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+synthesis)]

Liu et al. (13) reported the synthesis of ^99m^Tc-HYNIC-E{E[c(RGDfK)]_2_}_2_(tricine)(TPPTS) by incubation of 20 μg HYNIC-E{E[c(RGDfK)]_2_}_2_, 6.5 mg tricine, 5 mg TPPTS, and 1.85 GBq (50 mCi ) Na[^99m^TcO_4_] for 20-25 min at 100ºC. Radiochemical purity was >95%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+in+vitro)]

Using a receptor-binding assay with ^125^I-echistatin to α_v_β_3_ integrin receptors on cell surface of MDA-MB-435 human breast cancer cells, Liu et al. (13) reported that E{E[c(RGDfK)]_2_}_2_ and E[c(RGDfK)]_2_ had IC_50_ values of 51 ± 11 and 78 ± 27 nM, respectively. IC_50_ values for HYNIC-E{E[c(RGDfK)]_2_}_2_ and HYNIC-E[c(RGDfK)]_2_ were 55 ± 11 and 52 ± 9 nM, respectively. The in vitro solution stability of ^99m^Tc-HYNIC-E{E[c(RGDfK)]_2_}_2_(tricine)(TPPTS) was tested by incubating the radiolabeled peptide in buffer solution that contained 1.0 mg/ml cysteine at 37ºC for up to 12 h. No significant degradation of ^99^Tc-HYNIC-E{E[c(RGDfK)]_2_}_2_(tricine)(TPPTS) was observed under this condition.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+rodentia)]

Liu et al. (13) performed biodistribution studies of ^99m^Tc-HYNIC-E{E[c(RGDfK)]_2_}_2_(tricine)(TPPTS) in nude mice bearing MDA-MB-435 tumors. Tumor uptake was 5.60 ± 0.87% ID/g at 5 min after injection and increased to 7.30 ± 1.32% ID/g at 120 min. The uptakes of the tetramer in the tumor were significantly higher than that of the dimer (3.50% ID/g at 5 min and 3.82% ID/g at 120 min). Tumor/blood ratios were similar at all time points with highest at 24 h with a value of 63 for both compounds. At all time points, retention of the tetramer in the kidney (33.05% ID/g at 5 min and 25.93% ID/g at 120 min) was significantly higher as compared to the dimer (24.15% ID/g at 5 min and 14.33% ID/g at 120 min). Both peptides exhibited similar accumulation in the spleen, liver and lung. The tumor/blood, tumor/liver and tumor/lung ratios were significantly better than those of the dimer at 30-120 min after injection.

Co-injection of E-[c(RGDfK)]_2_ (30 mg/kg) with ^99m^Tc-HYNIC-E{E[c(RGDfK)]_2_}_2_(tricine)(TPPTS) resulted in a significant reduction of radioactivity in the tumor, lung, liver, spleen, and intestine. The radioactivity in the kidney and muscle was also slightly reduced. SPECT imaging in nude mice bearing MDA-MB-435 tumors with 15 MBq (0.41 mCi) of ^99m^Tc-HYNIC-E{E[c(RGDfK)]_2_}_2_(tricine)(TPPTS) revealed that the tumors were clearly visualized at 1, 2, and 4 h after injection with low radioactivity levels in the liver and lungs.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+human)]

No publication is currently available.

## NIH Support

R01 CA115883-01A2

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Liu S., Hsieh W.Y., Jiang Y., Kim Y.S., Sreerama S.G., Chen X., Jia B., Wang F. (2007). Evaluation of a (99m)Tc-labeled cyclic RGD tetramer for noninvasive imaging integrin alpha(v)beta3-positive breast cancer. Bioconjug Chem.